# (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2,3-dimethoxybenzamide

Chemical name: | (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2,3-dimethoxybenzamide
Abbreviated name: | [^18^F]Fallypride
Synonym:
Agent Category: | Compound
Target: | D_2/3_ dopamine receptors
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fallypride%5BAll%20Fields%5D)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_ through D_5_, have been well characterized pharmacologically and biochemically (4). These five subtypes are classified into two subfamilies: D_1_-like (D_1_ and D_5_) and D_2_-like (D_2_, D_3_, and D_4_) dopamine receptors. D_1_-like and D_2_-like receptors exert synergistic as well as opposite effects at both the biochemical and overall system level. A great majority of striatal D_1_ and D_2_ receptors are localized postsynaptically on caudate-putamen neurons and to a lesser extent presynaptically on nigrostiatal axons.

Substituted benzamides, such as sulpiride, raclopride, and iodobenzamide, are specific ligands with only moderate affinity for the D_2_ receptors, making studies of extrastriatal D_2_ receptors difficult (5-7). In binding studies, [^123^I]-labeled epidepride, an analog of isoremoxipride, was found to have high potency and low nonspecific binding, and to be selective for striatal and extrastriatal D_2_ receptors (8). Epidepride has marginal binding to D_4_ receptors, with little affinity for other known neurotransmitter receptors. (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2,3-dimethoxybenzamide ([^18^F]fallypride), an analog of epidepride, was found to be a selective, high-affinity antagonist of D_2/3_ receptors (9), and in positron emission tomography (PET) in vivo studies (10-12), it identified extrastriatal D_2/3_ receptors. [^18^F]Fallypride PET has been used to study D_2/3_ receptor occupancy and density in neuropsychiatric disorders and aging in humans.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20Fallypride%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

[^18^F]fallypride is formed by nucleophilic fluorination of (S)-N-[(1-allyl-2-pyrrolidinyl)methyl]-5-(3-tosyloxypropyl)-2,3-dimethoxybenzamide with K[^18^F]F/Kryptofix2.2.2, with yields of 20-40% (EOS/EOB, decay corrected) and specific activities of 33.3-62.9 TBq/mmol (900-1700 Ci/mmol) after reverse-phase HPLC purification from EOB in 60 min (9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20Fallypride%5BAll%20Fields%5D%20AND%20in%20vitro)]

Fallypride was reported to have high binding affinities for D_2_ and D_3_ receptor sites in homogenates of rat striatal membranes (9, 13). The K_i_ for D_2_, obtained by use of [^125^I]-labeled epidepride, was 0.03 nM, and the IC_50_, obtained by use of [^3^H]spiperone, was 0.05 nM. In recombinant cell lines, fallypride exhibited a high affinity ([^3^H]spiperone, IC_50_, 0.30 nM) for D_3_ receptors and low affinity ([^3^H]spiperone, IC_50_, 240 nM) for D_4_ receptors. The K_d_ of [^18^F]fallypride for D_2_ was 0.033 nM when assayed at room temperature in rat striatal homogenates; however, the K_d_ in another study was 2.03 ± 1.07 nM at 37ºC (0.04 ± 0.03 nM at 22ºC) (14). The B_max_ for D_2/3_ receptors was found to be 16.6 pmol/g tissue in a study using [^125^I]-labeled epidepride in post mortem human putamen (15).

In vitro autoradiographic studies of rat brain slices with [^18^F]fallypride showed that the striatum exhibited the highest amounts of radioactivity, followed to a lesser extent by the extrastriatal regions (2-6% of the striatal accumulation), such as the hypothalamus, thalamus, amygdala, and substantia nigra (9, 13). Binding to these areas was blocked by 10 μM haloperidol (>95%) or 100 nM clozapine (>80%), indicating specific binding to D_2/3_ receptor sites.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20Fallypride%5BAll%20Fields%5D%20AND%20rodentia)]

Biodistribution studies in rats showed a high accumulation of radioactivity in the muscle [9.96% injected dose (ID)/organ], followed by the liver (3.19% ID/organ), bone (2.32% ID/organ), kidney (0.96% ID/organ), and brain (0.57% ID/organ) at 30 min after injection of [^18^F]fallypride (9). There was a marked accumulation of the tracer in the striata within the first 60 min (2.5% ID/g), followed by a slow decrease of radioactivity to 1.8% ID/g at 90 and 120 min. In contrast, radioactivity in the cerebellum, which is reported to contain minimal D_2/3_ receptors, decreased continuously from 30 min (0.120% ID/g) to 120 min (0.014% ID/g). The striatum-to-cerebellum ratios were 17.1, 42.4, 62.5, and 122.1 at 30, 60, 90, and 120 min, respectively. [^18^F]Fallypride thus displayed uptake and washout kinetics characteristic of reversible radiotracers. The various extrastriatal regions showed significant specific binding (0.04-0.085% ID/g) at 120 min. Haloperidol (1 mg/kg) effectively blocked specific binding of [^18^F]fallypride to the striata and other extrastriatal regions (9, 13). Clozapine (40 mg/kg) and risperidone (0.1 mg/kg) exhibited >90% receptor occupancy (16).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20Fallypride%5BAll%20Fields%5D%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20Fallypride%5BAll%20Fields%5D%20AND%20%28primate%20not%20human%29)]

[^18^F]Fallypride PET studies in non-human primates have provided useful assessment of the D_2_ receptor in the brain, showing localization of [^18^F]fallypride not only in striatal regions but also in extrastriatal areas, such as the hypothalamus, thalamus, amygdala, and substantia nigra (14, 16-19). Quantitative analysis of [^18^F]fallypride binding was usually performed with distribution volume (DV), distribution volume ratio (DVR, with cerebellum as reference), and various kinetic constants. In equilibrium analyses, K_d_ estimates were 0.22 ± 0.05 nM in the striatum, 0.17 ± 0.05 nM in the thalamus, and 0.21 ± 0.07 nM in the hippocampus, whereas B_max_ values were 27.20 ± 7.57 nM in the striatum, 2.49 ± 0.96 nM in the thalamus, and 2.36 ± 0.84 nM in the hippocampus (14). Using kinetic analyses, Christian et al. (17) estimated B_max_ values for the putamen (27 nM), caudate (23 nM), ventral striatum (14 nM), thalamus (1.8 nM), and amygdala (0.9 nM).

Mukherjee et al. (9) showed selective uptake in the striata (0.04-0.06% ID/cc) of rhesus monkey brains with striatum-to-cerebellum ratios of 3 at 14 min, 5 at 35 min, 8 at 70 min, and 10 at 100 min after injection. The striatal accumulation of [^18^F]fallypride was reversed by treatment with haloperidol (1 mg/kg) with a dissociation rate of 0.0385 min^-1^ (t_1/2_ = 18 min). In another PET study using monkeys, putamen exhibited the highest accumulation of [^18^F]fallypride (DV = 48.1) followed by the caudate (DV = 45.0), thalamus (DV = 4.77), temporal cortex (DV = 2.39), frontal cortex (DV = 2.22), and cerebellum (DV = 1.35) (16). Clozapine (9.7 mg/kg), risperidone (0.05 mg/kg), and haloperidol (0.05 mg/kg) exhibited D_2_ receptor occupancies of 70%, 75%, and 90%, respectively.

D-Amphetamine is known to induce a marked release of dopamine to the synaptic cleft (20). D-Amphetamine administration to monkeys (0.75-1.50 mg/kg) decreased [^18^F]fallypride binding by 14.2-16.8% in the striatum at 60 min after injection of the drug. [^18^F]Fallypride was able to detect the change in dopamine levels induced by D-amphetamine in that study.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fallypride%5BAll%20Fields%5D%20AND%20human)]

[^18^F]Fallypride PET studies of D_2/3_ receptor distribution in human brain have been reported, showing a major localization of radioactivity in the striata and a significant minor accumulation in the extrastriatal regions (10, 12, 21). Quantitative analysis of [^18^F]fallypride binding was usually performed by use of DVRs (with cerebellum as reference), from which binding potentials (BPs) were derived to measure receptor concentrations. Mukherjee et al. (21) reported on [^18^F]fallypride PET studies in 6 normal subjects (21-63 years of age). PET brain scans showed high accumulation of radioactivity in the putamen (BP = 19-37) and caudate (BP = 16-32), followed by the thalamus (BP = 2.5-4.0), pituitary (BP = 1.1-7.4), amygdala (BP = 1.7-3.0), colliculi (BP = 1.7-2.4), substantia nigra (BP = 1.1-1.9), temporal cortex (BP = 0.4-1.2), frontal cortex (BP = 0.2-0.4), and parietal cortex (BP = 0.15-0.63) at 60 to 80 min after injection of [^18^F]fallypride (2.59 MBq/kg or 0.07 mCi/kg) with a test-retest error of <10%. At 180 min post injection, 30-40% of [^18^F]fallypride radioactivity remained intact in blood. There was an age-dependent decrease (>10% per decade) of [^18^F]fallypride binding in all brain regions.

Grunder et al. (10) studied striatal and extrastriatal binding of [^18^F]fallypride for D_2/3_ receptor sites in 15 clozapine-treated patients (25-47 years of age) with schizophrenia and in 7 healthy control subjects (23-41 years of age). The clozapine-treated patients exhibited significantly lower BP values than the healthy controls in the inferior temporal cortex, thalamus, caudate, amygdala, substantia nigra, and putamen. The D_2/3_ receptor occupancy in the inferior temporal cortex, thalamus, caudate, amygdala, substantia nigra, and putamen was 55 ± 6%, 44 ± 4%, 43 ± 6, 43 ± 5, 42 ± 5, and 36 ± 5%, respectively. The receptor occupancy was significantly higher in the cortical than in the striatal regions (P < 0.005). The clozapine plasma EC_50_ concentration was higher in the putamen (950 ng/ml) than in the inferior temporal cortex (333 ng/ml). On the basis of their results, the authors concluded that clozapine binds preferentially to cortical receptors with 60% receptor occupancy with plasma concentration of 350-400 ng/ml, which corresponds to the threshold for antipsychotic efficacy of clozapine.

In a [^18^F]fallypride PET study of 6 schizophrenic patients treated with olanzapine and 6 treated with haloperidol, Kessler et al. (22) reported that occupancy of D_2/3_ receptors by olanzapine was not significantly different from that seen with haloperidol in the putamen, ventral striatum, medial thalamus, amygdala, or temporal cortex (67.5-78.2% occupancy). However, occupancy of D_2/3_ receptors in the substantia nigra/ventral legmental area (VTA) was significantly lower in olanzapine-treated (40.2 ± 12.2%) compared with haloperidol-treated patients (59.3 ± 9.2%). In olanzapine-treated patients, the substantia nigra/VTA (40.2 ± 12.2%) was the only region with significantly lower D_2/3_ receptor occupancy than the putamen (69.2 ± 10.2%). The authors concluded that sparing of substantia nigra/VTA D_2/3_ receptor occupancy may therefore contribute to the low incidence of extrapyramidal side effects in olanzapine-treated patients.

Riccardi et al. (12) reported that D-amphetamine administration (0.43 mg/kg) to 14 normal subjects (6 females and 8 males) 21-32 years of age decreased [^18^F]fallypride binding significantly in various regions in the brain at 3 h after injection of the drug, as measured by PET imaging. Greatest displacements were seen in the caudate (5.6%), substantia nigra (6.6%), ventral striatum (7.2%), and putamen (11.2%). Lesser displacements were seen in the thalamus (2.8%), temporal cortex (3.7%), and amygdala (4.4%). Significant correlations of regional DA release with cognition and sensation-seeking behavior were observed. Riccardi et al. (23) also reported that α-methyl-para-tyrosine (AMPT) administration (71.4 mg/kg in six doses) to 6 normal subjects (3 females and 3 males) 23-38 years of age decreased [^18^F]fallypride binding significantly in various regions in the brain at 3.5 h after injection of the drug, as measured by PET imaging. Greatest displacements were seen in the caudate (8.83%), ventral striatum (10.64%), putamen (11.20%), and substantia nigra (12.69%). Lesser displacements were seen in the temporal cortex (0.11%), amygdala (1.00%), and medial thalamus (3.83%). Hence, [^18^F]fallypride PET can be used to estimate D_2/3_ receptor occupancy in striatal and extrastriatal regions of the human brain.

## Supplemental Information

[Disclaimers]

Synthesis Protocol

Toxicology

Preclinical Pharmacology

Clinical Pharmacology

Animal Dosimetry

Human Dosimetry

## NIH Support

R01 MH60898-03, M01 RR00095, R01 MH660890, K02 MH01603-0, MH59342-01, CA09206, NS10205, AA10027, AA10079, IP50 AA1287001

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 Gehlert D.R., Wamsley J.K. (1984). Autoradiographic localization of [3H]sulpiride binding sites in the rat brain. Eur J Pharmacol.
6 Lidow M.S., Goldman-Rakic P.S., Rakic P., Innis R.B. (1989). Dopamine D2 receptors in the cerebral cortex: distribution and pharmacological characterization with [3H]raclopride. Proc Natl Acad Sci U S A.
7 Brucke T., Tsai Y.F., McLellan C., Singhanyom W., Kung H.F., Cohen R.M., Chiueh C.C. (1988). In vitro binding properties and autoradiographic imaging of 3-iodobenzamide ([125I]-IBZM): a potential imaging ligand for D-2 dopamine receptors in SPECT. Life Sci.
8 Kessler R.M., Ansari M.S., Schmidt D.E., de Paulis T., Clanton J.A., Innis R., al-Tikriti M., Manning R.G., Gillespie D. (1991). High affinity dopamine D2 receptor radioligands. 2. [125I]epidepride, a potent and specific radioligand for the characterization of striatal and extrastriatal dopamine D2 receptors. Life Sci.
9 Mukherjee J., Yang Z.Y., Das M.K., Brown T. (1995). Fluorinated benzamide neuroleptics--III. Development of (S)-N-[(1-allyl-2-pyrrolidinyl)methyl]-5-(3-[18F]fluoropropyl)-2, 3-dimethoxybenzamide as an improved dopamine D-2 receptor tracer. Nucl Med Biol.
10 Grunder G., Landvogt C., Vernaleken I., Buchholz H.G., Ondracek J., Siessmeier T., Hartter S., Schreckenberger M., Stoeter P., Hiemke C., Rosch F., Wong D.F., Bartenstein P. (2005). and The Striatal and Extrastriatal D2/D3 Receptor-Binding Profile of Clozapine in Patients with Schizophrenia. Neuropsychopharmacology.
11 Mukherjee J., Christian B.T., Narayanan T.K., Shi B., Collins D. (2005). Measurement of d-amphetamine-induced effects on the binding of dopamine D-2/D-3 receptor radioligand, 18F-fallypride in extrastriatal brain regions in non-human primates using PET. Brain Res.
12. Riccardi, P., R. Li, M.S. Ansari, D. Zald, S. Park, B. Dawant, S. Anderson, M. Doop, N. Woodward, E. Schoenberg, D. Schmidt, R. Baldwin, and R. Kessler, Amphetamine-Induced Displacement of [(18)F] Fallypride in Striatum and Extrastriatal Regions in Humans. Neuropsychopharmacology, 2005.
13 Mukherjee J., Yang Z.Y., Brown T., Lew R., Wernick M., Ouyang X., Yasillo N., Chen C.T., Mintzer R., Cooper M. (1999). Preliminary assessment of extrastriatal dopamine D-2 receptor binding in the rodent and nonhuman primate brains using the high affinity radioligand, 18F-fallypride. Nucl Med Biol.
14 Slifstein M., Hwang D.R., Huang Y., Guo N., Sudo Y., Narendran R., Talbot P., Laruelle M. (2004). In vivo affinity of [18F]fallypride for striatal and extrastriatal dopamine D2 receptors in nonhuman primates. Psychopharmacology (Berl).
15 Kessler R.M., Whetsell W.O., Ansari M.S., Votaw J.R., de Paulis T., Clanton J.A., Schmidt D.E., Mason N.S., Manning R.G. (1993). Identification of extrastriatal dopamine D2 receptors in post mortem human brain with [125I]epidepride. Brain Res.
16 Mukherjee J., Christian B.T., Narayanan T.K., Shi B., Mantil J. (2001). Evaluation of dopamine D-2 receptor occupancy by clozapine, risperidone, and haloperidol in vivo in the rodent and nonhuman primate brain using 18F-fallypride. Neuropsychopharmacology.
17 Christian B.T., Narayanan T., Shi B., Morris E.D., Mantil J., Mukherjee J. (2004). Measuring the in vivo binding parameters of [18F]-fallypride in monkeys using a PET multiple-injection protocol. J Cereb Blood Flow Metab.
18 Christian B.T., Narayanan T.K., Shi B., Mukherjee J. (2000). Quantitation of striatal and extrastriatal D-2 dopamine receptors using PET imaging of [(18)F]fallypride in nonhuman primates. Synapse.
19 Mukherjee J., Yang Z.Y., Lew R., Brown T., Kronmal S., Cooper M.D., Seiden L.S. (1997). Evaluation of d-amphetamine effects on the binding of dopamine D-2 receptor radioligand, 18F-fallypride in nonhuman primates using positron emission tomography. Synapse.
20 Seiden L.S., Sabol K.E., Ricaurte G.A. (1993). Amphetamine: effects on catecholamine systems and behavior. Annu Rev Pharmacol Toxicol.
21 Mukherjee J., Christian B.T., Dunigan K.A., Shi B., Narayanan T.K., Satter M., Mantil J. (2002). Brain imaging of 18F-fallypride in normal volunteers: blood analysis, distribution, test-retest studies, and preliminary assessment of sensitivity to aging effects on dopamine D-2/D-3 receptors. Synapse.
22 Kessler R.M., Ansari M.S., Riccardi P., Li R., Jayathilake K., Dawant B., Meltzer H.Y. (2005). Occupancy of striatal and extrastriatal dopamine d(2)/d(3) receptors by olanzapine and haloperidol. Neuropsychopharmacology.
23 Riccardi P., Baldwin R., Salomon R., Anderson S., Ansari M.S., Li R., Dawant B., Bauernfeind A., Schmidt D., Kessler R. (2008). Estimation of Baseline Dopamine D(2) Receptor Occupancy in Striatum and Extrastriatal Regions in Humans with Positron Emission Tomography with [(18)F] Fallypride. Biol Psychiatry.